# TA138-conjugated ^111^In nanoparticles

Chemical name: | TA138-conjugated ^111^In nanoparticles
Abbreviated name: | α_v_β_3_-targeted ^111^In/NP
Synonym:
Agent Category: | Compound
Target: | α_v_β_3_-integrin receptor
Target Category: | Receptor-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT) or planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Structure of TA138 (an α_v_β_3_ integrin receptor antagonist) that is conjugated to the nanoparticles.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Integrin+targeted+111In+nanoparticles)]

Integrins are a broad family of glycoprotein, transmembrane cell surface receptors that are formed by the association of an α and a β subunit. These receptors are involved in cell-matrix interactions and also play a role in cell signaling and migration (1, 2). Because of their role in cell migration, the α_v_β_3_ integrin (that binds proteins such as vitronectin, fibronectin, thrombospondin, collagen, osteopontin, etc.) is a target of interest for the investigation of cancer metastasis and angiogenesis (3). Normally this receptor is expressed at low levels on epithelial and mature endothelial cells, but the expression is significantly upregulated during wound repair, cancer metastasis, and in neoplastic tumor vasculature (4-6). However, the exact role of α_v_β_3_ integrin in angiogenesis is unclear because the inhibition of this receptor inhibits tumor angiogenesis, but knockout mice lacking the β_3_ integrins were shown to develop larger than normal and extremely vascularized tumors (7, 8).

Visualization of small solid tumors has often helped in early detection of cancer and resulted in a favorable prognosis for the patient (9). Using magnetic resonance imaging with nanoparticles (NP) that target the α_v_β_3_ integrin, investigators have obtained high-resolution images of even minute tumors, but this technique requires knowledge of the exact location of the tumor to set up the equipment for imaging (10). Although a variety of radiolabeled compounds such as peptides, antibodies, and other α_v_β_3_ integrin antagonists have been used to visualize tumors in animals, these radiochemicals have limitations because of nonspecific binding (11, 12). Perfluorocarbon NP was shown to biodistribute primarily to the reticuloendothelial organs (lungs, liver, and spleen), and Hu et al. investigated the use of these NP with a radionuclide payload to detect budding tumors and their vasculature in different regions of the body, including the brain, head, neck, prostate, and breasts (10). The investigators developed an α_v_β_3_ integrin anatagonist labeled with indium (^111^In) on a perfluorocarbon NP (α_v_β_3_-targeted ^111^In/NP) and used the NP to visualize neoplastic tumor vasculature (10). The α_v_β_3_ integrin antagonist used to prepare the α_v_β_3_-targeted ^111^In/NP was TA138 (known as 3-sulfon-N-[[4,7,10-tris(carboxymethyl)1,4,7,10-tetraaza-cyclododec-1-yl]acetyl]-L-alanyl-N-[2-[4-[[[(1S)-1-carboxy-2[[[1,4-dihydro-7-[(1H-imidazol-2-ylamino]methyl]-1-methyl-4-oxo-3-quinolinyl] carbonyl]amino]ethyl]amino]sulfonyl]-3,5-dimethylphenoxy]-1-oxobutyl]amino]ethyl]-3-sulfo-L-alaninamide) (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=perfluorocarbon+nanoparticles+synthesis)]

The perfluorocarbon NP were produced as detailed by Hu et al. (10). A mixture of perfluorooctylbromide (PFOB), a surfactant commixture, with glycerin and water was evaporated under reduced pressure and dried overnight at 50°C in a vacuum oven. The commixture consisted of lecithin, dipalmitoyl-L-α-ethanolamine, cholesterol, methoxy-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-caproyl-phosphatidylethanolamine and TA138 conjugated to polyethylene glycol 2000 dissolved in chloroform (13-15). The dried mixture was then suspended in water by sonication to produce a liposomal suspension (14). The liposomes were blended with PFOB and distilled, deionized water and emulsified at 20,000 psi for 4 minutes. The completed emulsion was aliquoted into a vial, sealed under nitrogen, and stored until use. The exact storage conditions were not provided in the publication. The NP size was determined with a laser light–scattering submicron particle size analyzer to be nominally 242 nm with a polydispersity index of 0.231 at 37°C (10).

The synthesis of TA138 was described by Liu et al. (16). For this, 2-{[(4-{3-[N-(2-{(2R)-2-[(2R)-3-sulfo-2-(2-{1,4,7,10-tetraaza-4,7,10-tris[(tert-butoxycarbonyl)methyl] cyclododecyl}acetylamino)propyl]-3-sulfopropyl}ethyl)carbamoyl]propoxy}-2,6-dimethylphenyl) sulfonyl]amino}(2S)-3-{[1-methyl-4-oxo-7-({[1-(triphenylmethyl)imidazol-2-yl]-amino}methyl)(3-hydroquinolyl)]carbonylamino}propanoic acid (DPC-AG1613) was dissolved in trifluoroacetic acid and triethylsilane, heated at 70°C under nitrogen for 60 min, and concentrated under vacuum to obtain an oily solid. The solid was partitioned between diethyl ether and aqueous acetonitrile (ACN). The ether layer was once again extracted with aqueous ACN, and the two aqueous extractions were pooled for freeze-drying to obtain crude TA138 (16). Pure TA138 was obtained by several runs of the crude preparation on high-performance liquid chromatography using a Vydac C_18_ pharmaceutical column. The salt was subsequently extracted in ACN and water and then freeze-dried to obtain pure TA138 as a fluffy solid (16).

Coupling of ^111^In to α_v_β_3_ integrin–targeted perfluorocarbon NP was done at two different concentrations of the radionuclide (to produce particles with ~1 and ~10 radionuclides per NP, respectively), and it was achieved in citrate buffer (pH 5.7) (10). Briefly, α_v_β_3_ integrin–targeted perfluorocarbon NP was combined with [^111^In]indium chloride (in hydrochloric acid) in citrate buffer and incubated overnight at 40°C in a shaker water bath. The reaction was stopped by adding free diethylenetriamine pentaacetic acid for 5 min to remove all the free ^111^In. Coupling efficiency was determined by thin-layer chromatography at room temperature. It ranged from 50% to 70% for the ~10 nuclides/NP and 85% to 90% for the ~1 nuclide/NP. The specific activity and radiochemical purity of the final product were not reported by the investigators (10)

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%CE%B1v%CE%B23+integrin-targeted+perfluorocarbon+NP+in+vitro)]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%CE%B1v%CE%B23+integrin-targeted+perfluorocarbon+NP+rodentia)]

No publications are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%CE%B1v%CE%B23+integrin-targeted+perfluorocarbon+NP+Non-Primate+Mammals)]

Hu et al. investigated in vivo angiogenesis in 15 New Zealand rabbits bearing Vx-2 carcinoma tumors (10). The rabbits were divided into five groups and administered the respective ~10 ^111^In/NP α_v_β_3_ integrin–targeted (n = 3) or the ~1 ^111^In/NP α_v_β_3_ integrin–targeted (n = 4) preparations. The control rabbits (n = 4) received non-targeted ^111^In/NP, and for the competition study a group of animals (n = 4) received an excess of non-radioactive α_v_β_3_-targeted NP, along with α_v_β_3_-targeted ~10 ^111^In/NP at a ratio of 3:1. The control animals received non-targeted NP as either ~10 ^111^In/NP (n = 2) or ~1 ^111^In/NP (n = 2). The animals were examined 18 and 48 h after administration to assess persistence of the label. From planar images it was clear that the tumor contrast in animals injected with the α_v_β_3_-targeted NP was higher than in animals injected with the non-targeted preparation. On average, animals injected with the targeted formulation had approximately four times higher (P < 0.05; 0.48 ± 0.05% of the injected dose (ID)) accumulation of radioactivity in the tumors compared to the animals that received the non-targeted dose (0.10 ± 0.06% ID).

Imaging of the tumor neovasculature was performed up to 2 h after administration of α_v_β_3_-targeted ^111^In/NP bearing ~10 ^111^In/NP and compared with animals receiving three-fold more unlabeled α_v_β_3_-targeted NP. During the 2-h period, the tumor/muscle ratio (TMR) of animals injected with the radiolabeled ligand averaged to 6.3 ± 0.2 compared with an average TMR of 4.1 ± 0.2 observed in animals injected with the unlabeled ligand. This difference was reported to persist over the entire 2 h of imaging. A similar difference and persistence in TMR was observed between animals that received the ~10 ^111^In/NP and ~1 ^111^In/NP α_v_β_3_-targeted doses.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%CE%B1v%CE%B23+integrin-targeted+perfluorocarbon+NP+Non-Human+Primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=%CE%B1v%CE%B23+integrin-targeted+perfluorocarbon+NP+Human)]

No publications are currently available.

## References

1 Chan K.T., Cortesio C.L., Huttenlocher A. (2007). Integrins in cell migration. Methods Enzymol.
2 Lad Y., Harburger D.S., Calderwood D.A. (2007). Integrin cytoskeletal interactions. Methods Enzymol.
3 Barrett T., Brechbiel M., Bernardo M., Choyke P.L. (2007). MRI of tumor angiogenesis. J Magn Reson Imaging.
4 Cai W., Chen X. (2006). Anti-angiogenic cancer therapy based on integrin alphavbeta3 antagonism. Anticancer Agents Med Chem.
5 Honda Y., Kitano T., Fukuya F., Sato Y., Iwama S., Morie T., Notake M. (2005). A Novel alphavbeta3 integrin antagonist suppresses neointima formation for more than 4 weeks after balloon injury in rats. Arterioscler Thromb Vasc Biol.
6 Zhao Y., Bachelier R., Treilleux I., Pujuguet P., Peyruchaud O., Baron R., Clement-Lacroix P., Clezardin P. (2007). Tumor alphavbeta3 integrin is a therapeutic target for breast cancer bone metastases. Cancer Res.
7 Kumar C.C., Malkowski M., Yin Z., Tanghetti E., Yaremko B., Nechuta T., Varner J., Liu M., Smith E.M., Neustadt B., Presta M., Armstrong L. (2001). Inhibition of angiogenesis and tumor growth by SCH221153, a dual alpha(v)beta3 and alpha(v)beta5 integrin receptor antagonist. Cancer Res.
8 Reynolds L.E., Wyder L., Lively J.C., Taverna D., Robinson S.D., Huang X., Sheppard D., Hynes R.O., Hodivala-Dilke K.M. (2002). Enhanced pathological angiogenesis in mice lacking beta3 integrin or beta3 and beta5 integrins. Nat Med.
9 Elkin E.B., Hudis C., Begg C.B., Schrag D. (2005). The effect of changes in tumor size on breast carcinoma survival in the U.S.: 1975-1999. Cancer.
10 Hu G., Lijowski M., Zhang H., Partlow K.C., Caruthers S.D., Kiefer G., Gulyas G., Athey P., Scott M.J., Wickline S.A., Lanza G.M. (2007). Imaging of Vx-2 rabbit tumors with alpha(nu)beta3-integrin-targeted 111In nanoparticles. Int J Cancer.
11 Knight L.C., Romano J.E., Cosenza S.C., Iqbal N.M., Marcinkiewicz C. (2007). Differences in binding of (99m)Tc-disintegrins to integrin alphavbeta3 on tumor and vascular cells. Nucl Med Biol.
12 Shin I.S., Jang B.S., Danthi S.N., Xie J., Yu S., Le N., Maeng J.S., Hwang I.S., Li K.C., Carrasquillo J.A., Paik C.H. (2007). Use of antibody as carrier of oligomers of peptidomimetic alphavbeta3 antagonist to target tumor-induced neovasculature. Bioconjug Chem.
13 Harris T.D., Kalogeropoulos S., Nguyen T., Liu S., Bartis J., Ellars C., Edwards S., Onthank D., Silva P., Yalamanchili P., Robinson S., Lazewatsky J., Barrett J., Bozarth J. (2003). Design, synthesis, and evaluation of radiolabeled integrin alpha v beta 3 receptor antagonists for tumor imaging and radiotherapy. Cancer Biother Radiopharm.
14 Lanza G.M., Wallace K.D., Scott M.J., Cacheris W.P., Abendschein D.R., Christy D.H., Sharkey A.M., Miller J.G., Gaffney P.J., Wickline S.A. (1996). A novel site-targeted ultrasonic contrast agent with broad biomedical application. Circulation.
15 Winter P.M., Caruthers S.D., Kassner A., Harris T.D., Chinen L.K., Allen J.S., Lacy E.K., Zhang H., Robertson J.D., Wickline S.A., Lanza G.M. (2003). Molecular imaging of angiogenesis in nascent Vx-2 rabbit tumors using a novel alpha(nu)beta3-targeted nanoparticle and 1.5 tesla magnetic resonance imaging. Cancer Res.
16 Liu S., Harris T.D., Ellars C.E., Edwards D.S. (2003). Anaerobic 90Y- and 177Lu-labeling of a DOTA-conjugated nonpeptide vitronectin receptor antagonist. Bioconjug Chem.